# ^111^In-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-anti-insulin-like growth factor 1 receptor Affibody Z_IGF1R:4551_

Chemical name: | ^111^In-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-anti-insulin-like growth factor 1 receptor Affibody Z_IGF1R:4551_
Abbreviated name: | ^111^In-DOTA-Z_IGF1R:4551_
Synonym: | ^111^In-[MMA-DOTA-Cys]-Z_IGF-1R:4551_
Agent category: | Antibody fragment, Affibody
Target: | Insulin-like growth factor 1 receptor (IGF-1R)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ZIGF-1R:4551)]

Insulin-like growth factor 1 (IGF-1, 70 amino acids) is secreted by the liver and target tissues in response to growth hormone stimulation (1). IGF-1 plays an important role in cell growth and development. IGF-1 binds to IGF-1 receptor (IGF-1R) with ~1,000-fold higher affinity than to insulin receptor. IGF-1R is a transmembrane tyrosine kinase receptor that is highly expressed in many human cancers (2). IGF-1R plays an important role in tumor proliferation, apoptosis, angiogenesis, and metastasis (3, 4). Triple-negative breast tumors are negative for estrogen receptors, progesterone receptors, and epidermal growth factor receptor-2 (HER2). Patients with triple-negative breast tumors have a lower survival rate than patients with estrogen receptor- or HER2-positive breast tumors (5). IGF-1R is overexpressed in 36% of all triple-negative breast carcinomas (6).Therefore, monitoring of IGF-1R expression in breast tumor lesions with a noninvasive imaging modality is important for development of therapeutic treatments of these patients with anti-IGF-1R monoclonal antibodies (7). The human anti-IGF-1R monoclonal antibody R1507 is directed against the extracellular domain of human IGF-1R (8). However, the pharmacokinetics of intact radiolabeled mAbs, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab')_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2 was constructed based on the 58-amino-acid Z-domain residues from one of the IgG-binding domains of staphylococcal protein A (9). Affibody molecules exhibit high binding affinity to HER2 with K_d_ values of <1 nM. Various radiolabeled Affibody molecules have been studied in terms of their ability to image HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. A new Affibody with site-specific cysteine at the C-terminus for labeling, Z_IGF1R:4551_, has been identified to bind to IGF-1R with high affinity (10). 1,4,7,10-Tetraazacyclododecane-1,4,7-tris-acetic acid-10-maleimidoethylacetamide (MMA-DOTA) chelator was used for ^111^In labeling of Z_IGF1R:4551_. ^111^In-[MMA-DOTA-Cys]-Z_IGF-1R:4551_ (^111^In-DOTA-Z_IGF-1R:4551_) was evaluated in nude mice bearing human prostate DU-145 tumors.

### Related Resource Links:

- Chapters in MICAD (IGF-1R (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=IGF-1R%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (IGF-1R (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=3480))
- Articles in Online Mendelian Inheritance in Man (OMIM) (IGF-1R (http://www.ncbi.nlm.nih.gov/omim/147370))
- Clinical trials (IGF-1R (http://www.clinicaltrials.gov/ct2/results?term=IGF1R))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R1507%20and%20synthesis)]

Affibody Z_IGF-1R:4551_ was reduced with dithiothreitol in 0.02 M ascorbic acid for 18 h at 37°C (10). The reduced Z_IGF-1R:4551_ was incubated with MMA-DOTA in 1:1 molar ratio in ammonium acetate buffer (pH, 5.5) for 18 h at 37°C. MMA-DOTA-Z_IGF-1R:4551_ was isolated with column chromatography. MMA-DOTA-Z_IGF-1R:4551_ (10 nmol) was mixed with 60 MBq (1.6 mCi) ^111^InCl_3_ and incubated for 30 min at 90°C. The labeling efficiency of ^111^In incorporation was >99%. Specific activity of the preparation was ~6 GBq/µmol (162 mCi/µmol). ^111^In-DOTA-Z_IGF-1R:4551_ was found to be stable after incubation for 4 h in the presence of 1,000-fold molar excess of EDTA.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R1507%20and%20in%20vitro)]

Tolmachev et al. (10) reported that Z_IGF-1R:4551_ exhibited an affinity constant (K_d_) of 500 ± 70 pM with MCF-7 cells using flow cytometry. ^111^In-DOTA-Z_IGF-1R:4551_ saturation binding studies with DU-145 cells and DOTA-Z_IGF-1R:4551_ (displacement ligand) showed that there were 25,000 ± 3,000 receptor sites per cells. Cell binding and internalization of ^111^In-DOTA-Z_IGF-1R:4551_ (1.5 nM) were determined at 1–4 h of incubation with DU-145 cells at 37°C. Cell-associated radioactivity reached a plateau after 1 h, whereas internalization of ^111^In-DOTA-Z_IGF-1R:4551_ gradually increased with time of incubation from 25% at 1 h to 35% of total cellular radioactivity at 4 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R1507%20and%20rodentia)]

Tolmachev et al. (10) performed ex vivo biodistribution studies in normal mice (n = 4/group) at 4 h after intravenous injection of 0.025 MBq (0.00067 mCi) ^111^In-DOTA-Z_IGF-1R:4551_. The kidney showed the highest accumulation of radioactivity with 40% injected dose/gram (ID/g), followed by the liver (4% ID/g), salivary gland (3% ID/g), lung (2% ID/g), spleen (<2% ID/g), pancreas (<2% ID/g), and stomach (<1% ID/g). The blood radioactivity level was 0.5% ID/g. Co-injection of DOTA-Z_IGF-1R:4551_ (1.6 nmol) lowered the radioactivity levels in the pancreas, lung, stomach, and salivary gland (P < 0.05), organs known to be rich in IGF-1R.

Tolmachev et al. (10) performed ex vivo biodistribution studies in nude mice (n = 4/group) bearing DU-145 xenografts at 1–24 h after injection of 0.025 MBq (0.00067 mCi) ^111^In-DOTA-Z_IGF-1R:4551._ The maximum accumulation of radioactivity in all tissues studied was observed at 1 h after injection. There was a rapid clearance from the blood and lung, whereas the radioactivity levels remained almost constant in the kidney, muscle, and bone. There was a slight washout from the tumors, pancreas, salivary gland, spleen, and stomach. The tumor/blood ratios were 1.2, 2.5, and 5.2 at 1, 4, and 24 h after injection, respectively. Co-injection of 50 nmol DOTA-Z_IGF-1R:4551_ decreased the tumor/blood ratio to ~1 at 4 h after injection. Planar gamma imaging showed a clear visualization of the tumors with the tumor/contralateral site ratio of 2.9 at 8 h after injection. The kidneys, liver, and salivary gland were also visualized.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R1507%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R1507%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R1507%20and%20human)]

No publication is currently available.

## References

1 Hernandez-Sanchez C., Blakesley V., Kalebic T., Helman L., LeRoith D. (1995). The role of the tyrosine kinase domain of the insulin-like growth factor-I receptor in intracellular signaling, cellular proliferation, and tumorigenesis. J Biol Chem.
2 LeRoith D., Werner H., Neuenschwander S., Kalebic T., Helman L.J. (1995). The role of the insulin-like growth factor-I receptor in cancer. Ann N Y Acad Sci.
3 Baserga R., Resnicoff M., Dews M. (1997). The IGF-I receptor and cancer. Endocrine.
4 Rosenzweig S.A., Atreya H.S. (2010). Defining the pathway to insulin-like growth factor system targeting in cancer. Biochem Pharmacol.
5 Carey L.A., Dees E.C., Sawyer L., Gatti L., Moore D.T., Collichio F., Ollila D.W., Sartor C.I., Graham M.L., Perou C.M. (2007). The triple negative paradox: primary tumor chemosensitivity of breast cancer subtypes. Clin Cancer Res.
6 Lerma E., Peiro G., Ramon T., Fernandez S., Martinez D., Pons C., Munoz F., Sabate J.M., Alonso C., Ojeda B., Prat J., Barnadas A. (2007). Immunohistochemical heterogeneity of breast carcinomas negative for estrogen receptors, progesterone receptors and Her2/neu (basal-like breast carcinomas). Mod Pathol.
7 Zha J., O'Brien C., Savage H., Huw L.Y., Zhong F., Berry L., Lewis Phillips G.D., Luis E., Cavet G., Hu X., Amler L.C., Lackner M.R. (2009). Molecular predictors of response to a humanized anti-insulin-like growth factor-I receptor monoclonal antibody in breast and colorectal cancer. Mol Cancer Ther.
8 Gong Y., Yao E., Shen R., Goel A., Arcila M., Teruya-Feldstein J., Zakowski M.F., Frankel S., Peifer M., Thomas R.K., Ladanyi M., Pao W. (2009). High expression levels of total IGF-1R and sensitivity of NSCLC cells in vitro to an anti-IGF-1R antibody (R1507). PLoS One.
9 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
10 Tolmachev V., Malmberg J., Hofstrom C., Abrahmsen L., Bergman T., Sjoberg A., Sandstrom M., Graslund T., Orlova A. (2012). Imaging of Insulinlike Growth Factor Type 1 Receptor in Prostate Cancer Xenografts Using the Affibody Molecule 111In-DOTA-ZIGF1R:4551. J Nucl Med.